# ^111^In/^86^Y-Labeled F(ab')_2_ fragment of panitumumab, a fully human monoclonal antibody directed against the extracellular domain III of the epidermal growth factor receptor

Chemical name: | ^111^In/^86^Y-Labeled F(ab')_2_ fragment of panitumumab, a fully human monoclonal antibody directed against the extracellular domain III of the epidermal growth factor receptor
Abbreviated name: | [^111^In/^86^Y]-CHX-A''-Panitumumab F(ab')_2_
Synonym:
Agent Category: | Antibody
Target: | Epidermal growth factor receptor (EGFR) extracellular domain III
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging; positron emission tomography (PET)
Source of signal / contrast: | ^111^In (SPECT); ^86^Y (PET)
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=panitumumab&cmd=DetailsSearch)]

Panitumumab (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=e0fa4bca-f245-4d92-ae29-b0c630a315c2) is a fully human anti-epidermal growth factor receptor (EGFR) monoclonal antibody (mAb; ~150 kD) that has been approved by the United States Food and Drug Administration (FDA) for the treatment of metastatic colorectal cancers (http://cancer.gov/cancertopics/wyntk/colon-and-rectal) that express the EGFR and are unresponsive to chemotherapy (1). This mAb has a very high affinity for the extracellular domain III of the EGFR. The general characteristics of panitumumab have been described by Argiles et al. (2), and its mode of action has been illustrated by Dubois and Cohen (1). The fully human mAb is well tolerated by individuals, slows disease progression, and improves the progression-free survival of patients (3). Therefore, [^111^In]-labeled panitumumab ([^111^In]-panitumumab) has been evaluated for the noninvasive detection of EGFR-positive tumors in an effort to screen for patients who would benefit from radioimmunotherapy with this mAb after it was labeled with a suitable radionuclide (3). ^64^Cu-Labeled panitumumab has been evaluated for use with positron emission tomography (PET) to detect head and neck squamous cell carcinoma xenograft tumors (these tumors expressed high levels of the EGFR) in mice, and it was shown that only low levels of the labeled mAb accumulated in the lesions (4). The investigators attributed the low uptake of the radiolabeled mAb by the tumors to poor vascular permeability of the lesions. In other studies, PET with ^86^Y-labeled panitumumab has been shown to detect HER1-positive tumors in mice (5). It has also been shown that the ability of [^86^Y]-panitumumab to determine the HER1 status of malignant mesothelioma in mice was superior to that of [^86^Y]-cetuximab (6).

In general, intact mAbs are not the best agents for noninvasive imaging of solid tumors because they have a large diameter and cannot penetrate easily into the lesions (7). In addition, the tumor-targeting ability of large mAbs may be compromised due to the development of an immune response in the animal or patient (for more details, see Scott et al. (8)). To circumvent these problems, investigators reduced the size of the mAbs by enzymatic digestion and removed the Fc portion of the molecules to produce bivalent F(ab')_2_ fragments (110 kD; for an illustration and other characteristics of the F(ab')_2_ fragments, see Kaur et al. (9)). Briefly, the most important characteristic of the F(ab')_2_ fragments is that they have low, nonspecific binding and show superior pharmacokinetic and tumor penetration properties compared with the intact mAb (7). On the basis of information presented above, the F(ab')_2_ fragments of panitumumab were generated and labeled with either ^111^In or ^86^Y (7). The biodistribution patterns of [^111^In]-panitumumab F(ab')_2_ and [^86^Y]-panitumumab F(ab')_2_ were then studied in nude mice bearing HER1-positive LS-174T cell (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CL-188&Template=cellBiology) tumors (7). The ^111^In- and ^86^Y-labeled fragments were also evaluated with single-photon emission computed tomography (SPECT) and PET imaging, respectively for the detection of these tumors.

### Related Resource Links

Panitumumab-related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books?term=Panitumumab%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D&cmd=DetailsSearch)

EGFR-related chapters (http://www.ncbi.nlm.nih.gov/books/?term=EGFR+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books) in MICAD

Pathways related to EGFR (http://pid.nci.nih.gov/search/intermediate_landing.shtml?molecule=EGFR&Submit=Go) (in Pathways Interaction Database)

EGFR in Online Mendelian Inheritance in Man Database (OMIM (http://omim.org/entry/131550))

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Panitumumab) with panitumumab

Other anti-EGFR antibodies approved for clinical use by the FDA (cetuximab (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=8bc6397e-4bd8-4d37-a007-a327e4da34d9), trastuzumab (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=492dbdb2-077e-4064-bff3-372d6af0a7a2))

EGFR tyrosine kinase inhibitors [PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=EGFR%20tyrosine%20kinase%20inhibitors&cmd=DetailsSearch)]

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-labeled%20panitumumab%20F%28ab%27%292%20fragment%20synthesis&cmd=DetailsSearch)]

Panitumumab was obtained from a biopharmaceutical company, and the F(ab')_2_ fragments of the mAb were generated by peptic digestion as described by Wong et al. (7). The F(ab')_2_ fragments were then conjugated with a rigid analog of diethylenetriamine pentaacetic acid (CHX-A''-DTPA), a bifunctional chelating agent, for labeling with ^111^In or ^86^Y. The bifunctional chelating agents were conjugated with the F(ab')_2_ fragments at molar excess chelating agent:F(ab')_2_ ratios of 5:1, 10:1, and 20:1, and the average chelate:protein ratios of the conjugates obtained from the reactions were 2.9, 1.7, and 5.6, respectively. Each of the immunoconjugates was then labeled with ^111^In as described elsewhere (10). The labeling efficiency of the reaction ranged from 13.9% to 49.4%, and specific activity of the radiolabeled conjugates ranged from 51.3 to 399.6 MBq/6.66 pmol (from 1.9 to 14.8 μCi/6.66 pmol) (7). The radiochemical yield (RCY), radiochemical purity (RCP), and stability of [^111^In]-panitumumab F(ab')_2_ were not reported.

The panitumumab F(ab')2 fragments were also labeled with ^86^Y ([^86^Y]-panitumumab F(ab')_2_) for use in PET imaging studies (7). However, the RCY, RCP, stability, and specific activity of [^86^Y]-panitumumab F(ab')_2_ were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-labeled%20panitumumab%20F%28ab%27%292%20fragment%20in%20vitro&cmd=DetailsSearch)]

Using purified human EGFR as the target, the immunoreactivities of the [^111^In]-panitumumab F(ab')_2_ fragments with the different chelate:mAb ratios were determined in a radioimmunoassay (7). With these fragments, the amount of radioactivity bound to the human receptor ranged from 54.7% to 59.5% of the total radioactivity added to the assay. Addition of 66.66 pmol nonradioactive F(ab')_2_ fragment to the assay reduced the binding to an average of 3.5%, indicating that the labeled panitumumab fragments had a binding specificity for the human EGFR.

Using a competition radioimmunoassay with ^125^I-labeled panitumumab as the ligand, the immunoconjugates with chelate:mAb ratios of 2.9, 1.7, and 5.6 had IC_50_ values of 0.6 nM, 0.7 nM, and 0.7 nM, respectively (7). These values were comparable to the 0.5 nM value obtained with the native panitumumab F(ab')_2_ fragment (7). This indicated that conjugation of CHX-A''-DTPA to the panitumumab F(ab')_2_ fragments had minimal effect on the immunoreactivity of the fragments (7). On the basis of this study, the panitumumab preparation with a chelate:mAb ratio of 1.7 was used for the biodistribution and imaging studies described below.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-labeled%20panitumumab%20F%28ab%27%292%20fragment%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^111^In]-panitumumab F(ab')_2_ fragments was investigated in athymic mice bearing subcutaneous (s.c.) or intraperitoneal (i.p.) lesions derived from LS-174T cells (7). The animals (n = 5 mice/time point) were injected with 202.5 MBq (7.5 μCi) [^111^In]-panitumumab F(ab')_2_ through the tail vein and euthanized at various time points ranging from 24 h to 168 h postinjection (p.i.). The major organs, including the tumors, were then harvested from the rodents to determine the amount of radioactivity accumulated in the different tissues. Results obtained from the study were presented as percent of injected dose per gram tissue (% ID/g). Among the various organs obtained from the animals, accumulation of radioactivity reached its maximum (13.13 ± 2.34% ID/g) in the kidneys at 24 h p.i. and decreased to 2.66 ± 0.46% ID/g by 168 h p.i. The liver showed an uptake of 8.01 ± 1.63% ID/g at 24 h p.i., which decreased to 3.38 ± 0.67% ID/g by 168 h p.i. At 24 h p.i., the blood had accumulated 6.84 ± 2.30% ID/g of the label, and this accumulation gradually decreased to 0.08 ± 0.02 by 168 h p.i. The amount of tracer in the tumors was 21.42 ± 7.67% ID/g at 24 h p.i., remained at this level up to 72 h p.i., and decreased to 8.01 ± 3.65% ID/g by 168 h p.i. All other organs showed a similar pattern of radioactivity uptake; i.e., the highest accumulation of the label was at 24 h p.i., followed by a gradual loss by 168 h p.i. No blocking studies were reported.

In another study, the use of [^111^In]-panitumumab F(ab')_2_ was evaluated for the targeting of s.c. LS-174T cell tumors in athymic mice (7). The mice (n = 5 animals/time point) with the s.c. tumors were given either an intravenous (i.v.) or an i.p. injection of the ^111^In-labeled F(ab')_2_ fragments as before. Animals from the different groups were euthanized at the time points mentioned above, and all major organs along with the tumors were removed to determine the level of tracer uptake in the various tissues. Results from this study showed that administration of [^111^In]-panitumumab F(ab')_2_ either through the i.v. or the i.p. route resulted in maximum uptake of the label in the tumors compared with other tissues. However, when the labeled panitumumab fragments were administered through the i.p. route, the accumulation of radioactivity in the lesions peaked at 48 h p.i. (~45.66% ID/g), whereas tumors in animals that received an i.v. injection showed maximum uptake at 72 h p.i. (~40.00% ID/g). No blocking studies were reported.

To evaluate the use of [^111^In]-panitumumab F(ab')_2_ fragments for the visualization of s.c. LS-174T cell tumors in the flank of athymic mice (n = 4 anesthetized animals), the rodents were administered ~2,700 MBq (100 μCi) of the radioimmunoconjugate through an i.v. injection (7). Planar scintigraphic images of the mice were acquired at 24, 48, 72, and 96 h p.i., and the tumors were visible in the images from 24 h p.i. to the end of the study period. From the images, it was evident that the radioactivity remained in the tumors for the entire duration of the experiment, and there was a simultaneous clearance of the tracer from the body. No blocking studies were reported.

To evaluate the use of [^86^Y]-panitumumab F(ab')_2_ as a radioimmunotherapeutic agent, mice bearing LS-174T xenografts (n = 2 anesthetized animals) were given an i.v. injection of ~2,700 MBq (100 μCi; ~20 pmol) of the tracer (7). PET images of the animals were acquired at 24 h and 48 h p.i (7). The tumors were clearly visible at both time points. Although the heart, lungs, and liver were also visible at the two time points, there appeared to be a reduced amount of radioactivity present in these organs at 72 h p.i., with a simultaneous increased accumulation of the label in the tumors. To determine the receptor binding specificity of [^86^Y]-panitumumab F(ab')_2_, mice (n = 2 animals) were injected with the radiolabeled conjugate in the presence of 666.66 pmol nonradioactive panitumumab F(ab')_2_ fragments, and PET images were acquired from the animals at 24 h and 48 h p.i (7). PET images acquired at 24 h p.i. showed a reduced accumulation of radioactivity in the tumors, and the amount of tracer present in the lesions was even lower at 72 h p.i. This clearly showed that [^86^Y]-panitumumab F(ab')_2_ fragments had a high specificity for binding to the EGFR. After completion of the imaging session, the animals were euthanized and the various organs were retrieved to correlate the uptake of radioactivity in the tissues with the PET images (7). A high correlation was observed between the % ID/cm^3^ calculated from the PET images and the ex vivo % ID/g tissue values obtained from the different tissues. Lowering the specific activity of [^86^Y]-panitumumab F(ab')_2_ by the addition of 100 pmol nonradioactive panitumumab F(ab')_2_ did not change the amount of radioactivity detected in the normal organs, blood, or tumors as determined with PET imaging or ex vivo quantitation.

From these studies, the investigators concluded that the panitumumab F(ab')_2_ fragments were suitable to target tumors that express HER1 in rodents (7).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-labeled%20panitumumab%20F%28ab%27%292%20fragment%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-labeled%20panitumumab%20F%28ab%27%292%20fragment%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-labeled%20panitumumab%20F%28ab%27%292%20fragment%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Work presented in this chapter was supported by the Intramural Research Program of the National Institutes of Health, National Cancer Institute, and the Center for Cancer Research.

## References

1 Dubois E.A., Cohen A.F. (2009). Panitumumab. Br J Clin Pharmacol.
2 Argiles G., Dienstmann R., Elez E., Tabernero J. (2012). Panitumumab: a summary of clinical development in colorectal cancer and future directions. Future Oncol.
3 Ray G.L., Baidoo K.E., Wong K.J., Williams M., Garmestani K., Brechbiel M.W., Milenic D.E. (2009). Preclinical evaluation of a monoclonal antibody targeting the epidermal growth factor receptor as a radioimmunodiagnostic and radioimmunotherapeutic agent. Br J Pharmacol.
4 Niu G., Li Z., Xie J., Le Q.T., Chen X. (2009). PET of EGFR antibody distribution in head and neck squamous cell carcinoma models. J Nucl Med.
5 Nayak T.K., Garmestani K., Baidoo K.E., Milenic D.E., Brechbiel M.W. (2010). Preparation, biological evaluation, and pharmacokinetics of the human anti-HER1 monoclonal antibody panitumumab labeled with 86Y for quantitative PET of carcinoma. J Nucl Med.
6 Nayak T.K., Garmestani K., Milenic D.E., Baidoo K.E., Brechbiel M.W. (2011). HER1-targeted 86Y-panitumumab possesses superior targeting characteristics than 86Y-cetuximab for PET imaging of human malignant mesothelioma tumors xenografts. PLoS One.
7 Wong, K.J., K.E. Baidoo, T.K. Nayak, K. Garmestani, M.W. Brechbiel, and D.E. Milenic, In Vitro and In Vivo Pre-Clinical Analysis of a F(ab')(2) Fragment of Panitumumab for Molecular Imaging and Therapy of HER1 Positive Cancers. EJNMMI Res, 2011. 1(1).
8 Scott A.M., Wolchok J.D., Old L.J. (2012). Antibody therapy of cancer. Nat Rev Cancer.
9 Kaur S., Venktaraman G., Jain M., Senapati S., Garg P.K., Batra S.K. (2012). Recent trends in antibody-based oncologic imaging. Cancer Lett.
10 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.